# ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-N,N’,N”,N’”-tetraacetic acid-GSC(succinimidopropionyl-EAYGWNleDF-NH_2_)-EAYGWNleDF-NH_2_

Chemical name: | ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-N,N’,N”,N’”-tetraacetic acid-GSC(succinimidopropionyl-EAYGWNleDF-NH_2_)-EAYGWNleDF-NH_2_ | [image]
Abbreviated name: | ^111^In-MGD5 | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | Gastrin/cholecystokinin subtype 2 receptor (CCK-2R) | [image]
Target Category: | Receptor | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^111^In | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of 111In-MGD5.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Gastrin%20cholecystokinin%20receptors&cmd=DetailsSearch)]

The gastrin/cholecystokinin subtype 2 receptor (CCK-2R) is a G-protein–coupled receptor (for structure, function, and pharmacology of CCK-2R, see Foucaud et al. (1)) that is believed to participate in the development of a variety of cancers and has a characteristic overexpression in the cancerous tumors (2, 3). As a consequence, investigators are interested in exploring the use of CCK-2R ligands, such as gastrin and cholecystokinin (and their derivatives), for the diagnostic imaging and possible therapy of cancers that overexpress this receptor (3-5). Cholecystokinin is the topic of several clinical trials (http://clinicaltrials.gov/ct2/results?term=cholecystokinin) around the world for the treatment of different gastrointestinal disorders and the diagnosis of pancreatic cancer. Several radiolabeled CCK-2R peptides have been evaluated under preclinical (3) and clinical conditions (6) for the visualization of CCK-2R–positive tumors, but the major limitation of using these peptides was reported to be either a high uptake by the kidneys or low accumulation in the tumors or both. During an earlier study, based on the tumor/kidney uptake ratio, an ^111^In-labeled analog of gastrin (^111^In-1,4,7,10-tetraazacyclododecane-N,N’,N”,N’”-tetraacetic acid (DOTA)-His-His-Glu-Ala-Tyr-Gly-Trp-Met-Asp-Phe-NH_2_ (H2-Met or APH070)) was shown to have a low kidney retention, but its uptake by the tumors was low (7). Also, multimerization of small-molecule receptor ligands is known to increase their affinity for the binding site (3), and radiolabeled dimeric and tetrameric cyclic Arg-Gly-Asp peptides have been used successfully to visualize α_v_β_3_ integrin receptors (8). On the basis of the observations described above, Sosabowski et al. (3) decided to evaluate a ^111^In-labeled dimeric form of APH070 (^111^In-DOTA-GSC(succinimidopropionyl-EAYGWNleDF-NH_2_)-EAYGWNleDF-NH_2_ (^111^In-MGD5)) for its in vitro characteristics (stability, cellular internalization, and receptor binding), biodistribution, and its use as an imaging agent for tumor visualization in mice bearing AR42J cell tumors (a rat amphicrine pancreatic acinar cell line (9)).

### Other sources of information regarding Gastrin/cholecystokinin subtype 2 receptor (CCK-2R)

Chapters on CCK-2R in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Gastrin%2Fcholecystokinin+receptor++AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad).

Information on gastrin/cholecystokinin receptors in OMIM (Online Mendelian Inheritance in Man) (http://www.ncbi.nlm.nih.gov/omim?term=Gastrin%2Fcholecystokinin%20receptor%20).

Human gastrin protein and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/L10822.1?ordinalpos=5&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) sequences.

Information on human cholecystokinin gene (http://www.ncbi.nlm.nih.gov/gene/885?ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-MGD5%20synthesis&cmd=DetailsSearch)]

The synthesis, purification, and ^111^In labeling of MGD5 have been described by Sosabowski et al. (3). The radiochemical yield, purity, and specific activity of the labeled compound were not reported. ^111^In-MGD5 was reported to be stable in mouse plasma at 37°C and remained 95% and ~90% intact at 5 h and 24 h, respectively, after exposure to plasma as determined with high-performance liquid chromatography (HPLC).

^111^In-APH070 was also synthesized for comparison studies with ^111I^n-MGD5 (3). The radiochemical yield, purity, and specific activity of ^111^In-APH070 were not reported. The stability of this labeled compound in human blood at 37°C was reported to be 95% at 4 h and 62% at 24 h (compared to 98% in phosphate-buffered saline) as determined with HPLC (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-MGD5%20in%20vitro&cmd=DetailsSearch)]

Competition receptor binding assays with increasing concentrations of non-radioactive MGD5 or APH070 were performed on AR24J cell membranes with^111^In-APH070 as the receptor ligand (3). MGD5 was shown to have a higher affinity for CCK-2R (50% inhibitory concentration (IC_50_) = 1.04 ± 0.16 nM) compared to an IC_50_ of 5.59 ± 1.46 nM for APH070. Using saturation binding assays with intact AR24J cells, the dissociation constants for ^111^In-MGD5 and ^111^In-APH070 were reported to be 0.69 ± 0.14 and 2.9 ± 0.6 nM, respectively (3). These studies indicated that MGD5 is a superior to APH070 as a ligand for CCK-2R.

The internalization rate of ^111^In-MGD5 by AR2J cells was almost twice that of ^111^In-APH070 (0.24%/min versus 0.14%/min) (3), and at 120 min after exposure to the labeled compounds, 31.1% and 16.7% of ^111^In-MGD5 and ^111^In-APH070 were respectively internalized by the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-MGD5%20rodentia&cmd=DetailsSearch)]

The biodistribution of ^111^In-MGD5 was studied in nude mice bearing AR24J cell tumors (n = 3 and 4 animals in two separate studies) and compared to the biodistribution of ^111^In-APH070 performed with two other groups (n = 4 and 5, respectively) of the same tumor-bearing mice (3). The labeled peptides were injected into the animals through the tail vein, and the mice were euthanized 4 h after injection. Major organs of the animals were harvested to determine the amount of accumulated radioactivity. The uptake of ^111^In-MGD5 (~5.5% of injected dose per gram tissue (% ID/g)) by the tumor was significantly higher (6-fold; P = 0.01) compared with that of ^111^APH070 (~0.90% ID/g). The kidney uptake of ^111^In-MGD5 was also higher (~3% ID/g) than ^111^In-APH070 (~1.5% ID/g). The tumor/kidney ratios for the two radiochemicals were 1.66 (for ^111^In-MGD5) and 0.6 (for ^111^In-APH070), indicating that the dimer was possibly superior to the monomer as an imaging agent. Static imaging (single-photon emission computer tomography/computed tomography (SPECT/CT) of mice (the number of animals used per imaging agent was not reported) respectively injected with the two radiochemicals confirmed the results obtained during the biodistribution investigation (3).

When the mice were co-injected with ^111^In-MGD5 in presence of excess (100 μg/animal) non-radioactive MGD5, the tumors were reported to show a 10-fold reduction in accumulation of the label, and the investigators concluded that uptake of the radiochemical was specific to the tumor (3).

Results obtained after SPECT/CT imaging of mice injected with either ^111^In-MGD5 (n = 1 animal) or ^111^In-APH070 (n = 1 animal) showed that accumulation of radioactivity in various organs of the mice was similar to that observed during the biodistribution studies (3). Dynamic SPECT imaging of the animals showed that there was a rapid uptake of both labeled compounds by the various organs and the tumors during the initial 5 min after the injection, followed by a gradual washout of radioactivity from the various tissues, including tumors. The clearance of ^111^In-APH070 from the different tissues was reported to be faster than that of ^111^In-MGD5. By 2 h after the injection, 89% of the labeled monomer had washed out from the tissues compared to 58% for the labeled dimer.

From these studies, the investigators concluded that ^111^In-MGD5 was a suitable ligand to target CCK-2R–overexpressing tumors in animals, but further evaluation in clinical trials is necessary before it can be used in humans (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-MGD5%20Non%20Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-MGD5%20Non%20Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-MGD5%20Human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## References

1 Foucaud M., Archer-Lahlou E., Marco E., Tikhonova I.G., Maigret B., Escrieut C., Langer I., Fourmy D. (2008). Insights into the binding and activation sites of the receptors for cholecystokinin and gastrin. Regul Pept.
2 Jin G., Ramanathan V., Quante M., Baik G.H., Yang X., Wang S.S., Tu S., Gordon S.A., Pritchard D.M., Varro A., Shulkes A., Wang T.C. (2009). Inactivating cholecystokinin-2 receptor inhibits progastrin-dependent colonic crypt fission, proliferation, and colorectal cancer in mice. J Clin Invest.
3 Sosabowski J.K., Matzow T., Foster J.M., Finucane C., Ellison D., Watson S.A., Mather S.J. (2009). Targeting of CCK-2 receptor-expressing tumors using a radiolabeled divalent gastrin peptide. J Nucl Med.
4 Black J.W. (2009). Reflections on some pilot trials of gastrin receptor blockade in pancreatic cancer. Eur J Cancer.
5 Reubi J.C., Maecke H.R. (2008). Peptide-based probes for cancer imaging. J Nucl Med.
6 Froberg A.C., de Jong M., Nock B.A., Breeman W.A., Erion J.L., Maina T., Verdijsseldonck M., de Herder W.W., van der Lugt A., Kooij P.P., Krenning E.P. (2009). Comparison of three radiolabelled peptide analogues for CCK-2 receptor scintigraphy in medullary thyroid carcinoma. Eur J Nucl Med Mol Imaging.
7 Mather S.J., McKenzie A.J., Sosabowski J.K., Morris T.M., Ellison D., Watson S.A. (2007). Selection of radiolabeled gastrin analogs for peptide receptor-targeted radionuclide therapy. J Nucl Med.
8 Liu S. (2006). Radiolabeled multimeric cyclic RGD peptides as integrin alphavbeta3 targeted radiotracers for tumor imaging. Mol Pharm.
9 Rosewicz S., Riecken E.O., Wiedenmann B. (1992). The amphicrine pancreatic cell line AR42J: a model system for combined studies on exocrine and endocrine secretion. Clin Investig.